# ^123^I-Labeled (S)-2-(3-((S)-1-carboxy-5-(4-iodobenzylamino)pentyl)ureido)pentanedoic acid

Chemical name: | ^123^I-Labeled (S)-2-(3-((S)-1-carboxy-5-(4-iodobenzylamino)pentyl)ureido)pentanedoic acid
Abbreviated name: | [^123^I]MIP-1072
Synonym: | ^123^I-Labeled (2S)-2-[[(2R)-1-hydroxy-6-[(4-iodanylphenyl)methylamino]-1-oxohexan-2- yl]carbamoylamino]pentanedioic acid
Agent Category: | Compound
Target: | Prostate-specific membrane antigen (PSMA) or glutamate carboxypeptidase II (GCP II) or folate hydrolase or N-acetylated-α-linked-acidic-dipeptidase (NAALADase)
Target Category: | Enzyme
Method of detection: | Single-photon emission computed tomography/computed tomography (SPECT/CT)
Source of signal / contrast: | ^123^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on above structure for additional information regarding [^123^I]MIP1072 in PubChem (http://pubchem.ncbi.nlm.nih.gov/deposit/deposit.cgi?s=submgr&ss=submarch&mid=265418). Click on protein (http://www.ncbi.nlm.nih.gov/protein/Q04609.1?ordinalpos=1&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum), nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NM_153696.2?ordinalpos=2&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=2346&log$=genesensor5&logdbfrom=nuccore) for additional information regarding the human PSMA.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MIP+1072)]

The prostate-specific membrane antigen (PSMA), a membrane-bound glycoprotein that possesses different peptidase activities (see Table above), is expressed mainly in the prostate epithelium. Because of its overexpression in primary, metastatic or hormone-refractory prostate and other cancers, including the neovasculature of solid tumors, this antigen is considered to be a cancer marker and a good target for imaging agents and therapy (1). Hence, PSMA has been targeted in several clinical trials (http://clinicaltrials.gov/ct2/results?term=PSMA) that have been approved by the United States Food and Drug Administration (FDA) for the treatment of prostate cancer. In addition, capromab pendetide, a commercially available monoclonal antibody (MAb) that binds to the intracellular domain of the PSMA and was approved by the FDA for the diagnostic imaging of prostate cancer (http://www.prostascintimaging.com./hcp/prostascint/), has limited use because the MAb binds primarily to necrotic parts of the tumor and may not detect any viable malignant tumor cells (2). Investigators have also developed and evaluated MAbs directed against the extracellular domains of PSMA, and after preclinical studies they reported that these MAbs could be of potential use in the detection and treatment of PSMA-positive cancers (3-5). However, results obtained from a phase I clinical trial to evaluate the use of ^111^In-labeled/unlabeled J591 MAb mixture to detect and target the PSMA-positive vasculature of progressive solid tumors in patients with breast, colon, liver, or kidney cancers showed that, although the antibody was well tolerated, selectively targeted a variety of solid tumors, but it did not yield any positive therapeutic response(s) (6). The investigators concluded that this was probably because the large molecular size of the MAb was a hindrance to its complete penetration into the tumors. In addition, therapeutic MAbs have poor pharmacokinetic profiles in normal tissues because they have an extended circulation period compared with the small molecule drugs.

Radiolabeled small molecule drugs have an advantage over MAbs because they are inexpensive to produce, can easily penetrate solid tumors, and, due to their pharmacokinetic properties, are superior for use in the detection (by imaging techniques) and therapy of cancerous tumors. On the basis of the facts presented above, a series of small-molecule inhibitors of PSMA were recently synthesized for possible use in conjunction with single-photon emission computed tomography/computed tomography (SPECT/CT) for the detection and staging of prostate cancer (7). Two of these compounds, (S)-2-(3-((S)-1-carboxy-5-(3-(4-iodobenzylamino)pentyl)ureido)pentanedoic acid (MIP-1072) and (S)-2-(3-((S)-1-carboxy-5-(3-(4-iodophenyl)ureido)pentyl)ureido)pentanedoic acid (MIP-1095), were labeled with ^123^I by Hillier et al. for evaluation as molecular imaging agents to detect prostate cancer in a mouse model (8). This chapter describes the studies performed with [^123^I]MIP-1072 under in vitro conditions and its biodistribution in mice bearing LNCaP (derived from human metastatic prostate carcinoma; expresses PSMA) and PC (developed from the bone marrow of a patient with secondary myelodisplastic syndrome; does not express PSMA; for further details regarding this cell line see (9)) cell xenograft tumors. Studies performed with [^123^I]MIP-1095 are presented in a separate chapter in MICAD (www.micad.nih.gov) (10).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+MIP-1072+synthesis)]

The synthesis and radioiodination of MIP-1072 was performed as described by Maresca et al. (7). The radiochemical yield was 50–70%, and purity of the labeled compound was reported to be >90%. Identity of the radioiodinated compound was confirmed with reverse-phase high-performance liquid chromatography (RP-HPLC) by co-injecting the tracer with its corresponding unlabeled compound. Specific activity of the iodinated compound was reported to be ≥148 MBq/μmol (≥4 Ci/μmol). [^123^I]MIP-1072 was reported to be stable at 40°C for at least 48 h as determined with RP-HPLC (7).

For comparative studies, [^123^I]MIP-1095 was also synthesized as above and had a similar yield, radiochemical purity, and specific activity as [^123^I]MIP-1072 (8). In addition, capromab pendetide was labeled with ^111^In to compare its biodistribution with [^123^I]MIP-1072 in xenograft mice. The specific activity of the ^111^In-labeled MAb was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+MIP+1072+in+vitro)]

Hillier et al. used LNCaP cells to determine the in vitro characteristics of [^123^I]MIP-1072 (8). Using [^3^H]-N-acetyl-aspartyl-glutamate as a substrate for N-acetylated-α-linked-acidic-dipeptidase (NAALADase), the inhibition constant (K_i_) of MIP-1072 was determined to be 4.6 ± 1.6 nmol/L (8). The dissociation constant (K_d_) and maximal binding (B_max_) of [^123^I]MIP-1072 for PSMA expressed on the LNCaP cells were reported to be 3.8 ± 1.3 nmol/L and 1,490 ± 60 fmol/10^6^ cells (0.9 × 10^6^ sites/cell), respectively. In addition, [^123^I]MIP-1072 was shown to be internalized by the LNCaP cells (8). The K_i_ and K_d_ values obtained with [^123^I]MIP-1072 were lower than those obtained with [^123^I]MIP-1095 (K_i_ and K_d_ were 0.24 ± 0.14 nmol/L and 0.81 ± 0.39 nmol/L, respectively); as expected, the B_max_ values obtained with both compounds were similar (10). The binding of [^123^I]MIP-1072 to LNCaP cells was shown to be inhibited (>95%) by 2-(phosphonomethyl)-pentanedioic acid (PMPA), a NAALADase inhibitor.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+MIP+1072+rodentia)]

The biodistribution of [^123^I]MIP-1072 was investigated in male NCr-nu/nu mice bearing LNCaP cell xenograft tumors (8). The animals were injected with the radiochemical through the tail vein and euthanized at predetermined time points (n = 5 mice/time point) varying from 15 min to 24 h after the treatment. The tumors and other important tissues were then collected from the animals to determine tracer uptake (expressed as percent injected dose/gram tissue (% ID/g)). By 24 h after treatment, the non-target tissues, including blood, had very low accumulation of radioactivity. At this time point a high amount of label was present in the tumor (5.03 ± 1.35% ID/g) followed by the kidneys (1.1 ± 0.60% ID/g; these organs have a high PSMA content). The tumors had a maximum amount of accumulated tracer (17.40 ± 6.30% ID/g) at 1 h after injection, and the uptake peaked in these organs (159 ± 46% ID/g) at 2 h after treatment. By comparison, the accumulation of [^123^I]MIP-1095 in the tumor and kidneys at 24 h was 29.10 ± 15.10% ID/g and 27.00 ± 26.20% ID/g, respectively. Unlike [^123^I]MIP-1072, the label from ^111^In-labeled capromab pendetide was present at higher levels in all the target and non-target organs even 72 h after the injection. The tumor/blood and tumor/skeletal muscle ratios were 411 and 64.5, 174 and 304 (at 24 h after the injection), and 2.92 and 41.2 (at 72 h after the injection) for [^123^I]MIP-1072, [^123^I]MIP-1095, and [^111^In] capromab pendetide, respectively (8). The investigators also noted that the clearance of [^123^I]MIP-1072 from the tumors was faster than that of [^123^I]MIP-1095 (P < 0.05). Also, there was no significant difference (P > 0.06) in the tumor levels of [^123^I]MIP-1095 between 1 h and 24 h after injection of the tracer. In general, compared with [^123^I]MIP-1072, a slower (P < 0.05) clearance of [^123^I]MIP-1095 was noted from the non-target tissues between 1 h and 8 h after the radiotracer injection. Although the brain contains a high level of NAALADase activity (11), little uptake of either [^123^I]MIP-1072 or [^123^I]MIP-1095 was observed in this organ, indicating that the radiochemicals did not cross the blood–brain barrier.

To investigate the in vivo binding specificity of [^123^I]MIP-1072 in mice bearing LNCaP tumors (n = 5 animals), the animals were injected with the radiochemical in the presence of excess PMPA (50 mg/kg animal body weight) and euthanized 2 h later (8). Under these conditions the accumulation of [^123^I]MIP-1072 in the tumors and kidneys was reported to be almost completely blocked, suggesting that accumulation of the radiochemical in these tissues was mediated by specific binding to PSMA.

Similar to the biodistribution studies, SPECT/CT imaging of mice bearing LNCaP (PSMA+ve), PC (PSMA-ve) or PC3 PIP (PC3 cells transfected with the PSMA gene) cell xenograft tumors 4 h after injection with [^123^I]MIP-1072 showed that the label accumulated primarily in the PSMA+ve tumors and the kidneys of the animals. This indicated the uptake of [^123^I]MIP-1072 was specific due to expression of PSMA on the cells and not as a consequence of blood flow or permeability differences between tumors derived from the different cell lines.

From these studies, the investigators concluded that both [^123^I]MIP-1095 and [^123^I]MIP-1072 could be developed for imaging, therapy (by attaching an appropriate nuclide to the molecules), and monitoring of prostate cancer in humans (8).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+MIP+1072+Non-Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+MIP+1072+Non-Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+MIP+1072+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No supplemental information is currently available.

## NIH Support

This work was supported by National Institutes of Health grants R43 EB004253, U24 CA92871, and R01 CA134675.

## References

1 Ghosh A., Heston W.D. (2004). Tumor target prostate specific membrane antigen (PSMA) and its regulation in prostate cancer. J Cell Biochem.
2 Troyer J.K., Beckett M.L., Wright G.L. (1997). Location of prostate-specific membrane antigen in the LNCaP prostate carcinoma cell line. Prostate.
3 Smith-Jones P.M., Vallabhajosula S., Navarro V., Bastidas D., Goldsmith S.J., Bander N.H. (2003). Radiolabeled monoclonal antibodies specific to the extracellular domain of prostate-specific membrane antigen: preclinical studies in nude mice bearing LNCaP human prostate tumor. J Nucl Med.
4 Vallabhajosula S., Goldsmith S.J., Kostakoglu L., Milowsky M.I., Nanus D.M., Bander N.H. (2005). Radioimmunotherapy of prostate cancer using 90Y- and 177Lu-labeled J591 monoclonal antibodies: effect of multiple treatments on myelotoxicity. Clin Cancer Res.
5 Milowsky M.I., Nanus D.M., Kostakoglu L., Sheehan C.E., Vallabhajosula S., Goldsmith S.J., Ross J.S., Bander N.H. (2007). Vascular targeted therapy with anti-prostate-specific membrane antigen monoclonal antibody J591 in advanced solid tumors. J Clin Oncol.
6 Morris M.J., Pandit-Taskar N., Divgi C.R., Bender S., O'Donoghue J.A., Nacca A., Smith-Jones P., Schwartz L., Slovin S., Finn R., Larson S., Scher H.I. (2007). Phase I evaluation of J591 as a vascular targeting agent in progressive solid tumors. Clin Cancer Res.
7 Maresca K.P., Hillier S.M., Femia F.J., Keith D., Barone C., Joyal J.L., Zimmerman C.N., Kozikowski A.P., Barrett J.A., Eckelman W.C., Babich J.W. (2009). A series of halogenated heterodimeric inhibitors of prostate specific membrane antigen (PSMA) as radiolabeled probes for targeting prostate cancer. J Med Chem.
8 Hillier S.M., Maresca K.P., Femia F.J., Marquis J.C., Foss C.A., Nguyen N., Zimmerman C.N., Barrett J.A., Eckelman W.C., Pomper M.G., Joyal J.L., Babich J.W. (2009). Preclinical evaluation of novel glutamate-urea-lysine analogues that target prostate-specific membrane antigen as molecular imaging pharmaceuticals for prostate cancer. Cancer Res.
9 Serrero G., Zhou J., Mills D., LePak N. (1991). Decreased transforming growth factor-beta response and binding in insulin-independent teratoma-derived cell lines with increased tumorigenic properties. J Cell Physiol.
10 Chopra, A., [123I]-Labeled (S)-2-(3-((S)-1-carboxy-5-(4-iodophenyl) ureido)pentyl)ureido)pentanedoic acid [123I]MIP-1095. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
11 Tiffany C.W., Lapidus R.G., Merion A., Calvin D.C., Slusher B.S. (1999). Characterization of the enzymatic activity of PSM: comparison with brain NAALADase. Prostate.